# Cy5.5-GGSGRSANAK(Fitc)C-poly-L-lysine-methoxy polyethylene glycol

Chemical name: | Cy5.5-GGSGRSANAK(Fitc)C-poly-L-lysine-methoxy polyethylene glycol
Abbreviated name: | Cy5.5-GGSGRSANAK(Fitc)C-PL-MPEG, Cy5.5-uPA-PGC
Synonym:
Agent category: | Peptide
Target: | Urokinase-type plasminogen activator
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on MMP-2 (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=116856) and MMP-9 (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=10443048) for protein information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=uPA+cy5%2E5)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play an important role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3). Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis (4-7).

Urokinase-type plasminogen activator (uPA) is a serine protease (8, 9). The uPA and uPA receptor (uPAR) system is responsible for tissue degradation after plasminogen activation to plasmin, which leads to a cascade of proteolysis or thrombolysis depending on the physiological conditions. uPA also directly activates MMPs, vascular endothelial growth factor, and human growth factor (10). Malignant tumors often express high levels of uPA and uPAR (11); therefore, the uPA/uPAR system is linked to vascular diseases and cancer. A synthetic, protected-graft copolymer (PGC), consisting of poly-L-lysine (PL) with multiple methoxy polyethylene glycol (MPEG) side chains, has been used as a drug carrier with efficient accumulation in tumors (12, 13). The peptide GGSGRSANAKC was found to be an uPA substrate that is cleaved between the Arg (R) and Ser (S) residues. Law et al. (14) used this sequence to attach a Cy5.5 near-infrared (NIR) dye molecule to the unmodified PL side chains of PGC to form Cy5.5-GGSGRSANAK(Fitc)C-PL-MPEG (Cy5.5-uPA-PGC), a fluorescence-quenched polymer. Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. The Cy5.5 molecules are in close proximity, which causes fluorescence quenching as a result of efficient fluorescence resonance energy transfer. The NIR fluorescence signal will increase when the Arg-Ser bond is cleaved by uPA, releasing fragments containing Cy5.5. Cy5.5-uPA-PGC is being developed for NIR fluorescence imaging of uPA proteolytic activity in tumors, atherosclerosis, myocardial infarction, and other diseases (15).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=uPA+cy5%2E5+synthesis)]

PL-MPEG was formed by reaction of the hydroxysuccinimde ester of MPEG succinate to the NH_2_ group of PL (35.5 kDa) (16). The purified PL-MPEG had a calculated average molecular mass of 480 kDa as determined with elemental analysis. The PL-MPEG was then iodoacetylated by reaction with excess iodoacetic acid. GGPRQITAGK(Fitc)C was coupled to the iodoacetylated PL-MPEG via a thiol-specific reaction at the C-terminal amino acid (C) (17). The resulting PGC was further modified with Cy5.5-hydroxysuccinimide ester via the free N-terminal amino acid (G) of the attached peptide. Cy5.5-MMP-PGC was purified with column chromatography. Each PL backbone contained an average of 92 MPEG molecules, 17–19 copies of GGPRQITAGK(Fitc)C peptide, and 15–19 Cy5.5 molecules.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=uPA+cy5%2E5+and+in+vitro)]

Law et al. (17) showed thatCy5.5-uPA-PGC (200 nM), a uPA substrate, was activated by uPA in a time-dependent manner with a six-fold increase in NIR fluorescence signal after 120 min of incubation. Co-incubation with amileride (uPA inhibitor) markedly reduced NIR fluorescence signal in a dose-dependent manner with a 50% inhibition concentration value of 63 µM. Hsiao et al. (15) showed that MMP-2, MMP-7, MMP-9, cathepsin B, and cathepsin D did not activate the uPA probe.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=uPA+cy5%2E5+rodentia)]

Hsiao et al. (15) performed reflectance fluorescence imaging studies of Cy5.5-uPA-PGC in mice bearing HT-1080 (n = 16) or HT-28 (n = 10) tumors. Images were obtained after injection of 10 nmol Cy5.5-uPA-PGC. The initial NIR signal in the HT-1080 tumors was 75 ± 1 arbitrary units (AU) at 0 h and increased to 735 ± 52 AU at 6 h and 1,206 ± 107 AU at 24 h. The NIR fluorescence signal in the HT-28 tumors was 935 ± 106 AU at 6 h and 1,217 ± 87 AU at 24 h. The tumor/muscle ratio for both tumors was 3.1–3.2 at 24 h. Histological immunofluorescence colocalized with immunoreactivity for uPA in the tumor sections. Zymography experiments also showed uPA expression in both tumor extracts. No blocking or uPA inhibition experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=uPA+cy5%2E5+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=uPA+cy5%2E5+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=uPA+cy5%2E5+human)]

No publication is currently available.

## NIH Support

P50 CA86355, R01 CA99385

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Choong P.F. Nadesapillai A.P. Urokinase plasminogen activator system: a multifunctional role in tumor progression and metastasis Clin Orthop Relat Res 2003Suppl415 S46 58 14600592
9 Rabbani S.A., Mazar A.P. (2001). The role of the plasminogen activation system in angiogenesis and metastasis. Surg Oncol Clin N Am.
10 Folkman J., Shing Y. (1992). and , Angiogenesis.
11 Duffy M.J., Maguire T.M., McDermott E.W., O'Higgins N. (1999). Urokinase plasminogen activator: a prognostic marker in multiple types of cancer. J Surg Oncol.
12 Marecos E., Weissleder R., Bogdanov A. (1998). Antibody-mediated versus nontargeted delivery in a human small cell lung carcinoma model. Bioconjug Chem.
13 Weissleder R., Cheng H.C., Marecos E., Kwong K., Bogdanov A. (1998). Non-invasive in vivo mapping of tumour vascular and interstitial volume fractions. Eur J Cancer.
14 Law B., Curino A., Bugge T.H., Weissleder R., Tung C.H. (2004). Design, synthesis, and characterization of urokinase plasminogen-activator-sensitive near-infrared reporter. Chem Biol.
15 Hsiao J.K., Law B., Weissleder R., Tung C.H. (2006). In-vivo imaging of tumor associated urokinase-type plasminogen activator activity. J Biomed Opt.
16 Weissleder R., Tung C.H., Mahmood U., Bogdanov A. (1999). In vivo imaging of tumors with protease-activated near-infrared fluorescent probes. Nat Biotechnol.
17 Chen J., Tung C.H., Allport J.R., Chen S., Weissleder R., Huang P.L. (2005). Near-infrared fluorescent imaging of matrix metalloproteinase activity after myocardial infarction. Circulation.